# 2'-Deoxy-2'-[^18^F]fluoro-1-β-D-arabinofuranosyl-adenine

Chemical name: | 2'-Deoxy-2'-[^18^F]fluoro-1-β-D-arabinofuranosyl-adenine
Abbreviated name: | [^18^F]FAA
Synonym:
Agent Category: | Compound
Target: | Unknown
Target Category: | Non-catabolized trapping inside cells
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2-fluoroadenosine)]

Adenylates are important in cellular metabolism and functions (1). Adenosine is converted intracellularly to adenosine triphosphate (ATP), which is an important source of energy as well as a regulator of cellular functions. Adenosine stimulates the acetylcholine-sensitive K^+^ current in the heart. Many fluorinated analogs of adenosine nucleoside have been investigated as potential antitumor and antiviral agents (2-5). 2'-Deoxy-2'-fluoro-9-β-D-arabinofuranosyl-adenine (FAA) has been reported to exhibit antitumor activity (6). [^18^F]FAA has been synthesized and studied in tumor-bearing mice with positron emission tomography (PET) imaging (7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2-fluoroadenosine+synthesis)]

Alauddin et al. (7) synthesized [^18^F]FAA by reaction of the respective triflate (N3,3’,5’-tri-methoxytrityl-2’-trifluoromethanesulfonyl-9-β-D-arabinofuranosyl-adenine) with tetrabutylammonium [^18^F]fluoride, followed by acid hydrolysis to remove the methoxytrityl protecting groups. The desired product, [^18^F]FAA, was purified with high-performance liquid chromatography with a radiochemical yield of 10%–12% (decay-corrected) and a radiochemical purity >99%. The average specific activity for [^18^F]FAA was >74 GBq/µmol (2,000 mCi/µmol) at the end of the synthesis. Total synthesis time was 90–95 min from the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2-fluoroadenosine+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2-fluoroadenosine+rodentia)]

Alauddin et al. (7) performed biodistribution studies of [^18^F]FAA in nude mice (n = 5) bearing an HT-29 tumor in the left flank and a herpes simplex virus thymidine kinase (HSV-tk)–transduced HT-29 tumor in the right flank. [^18^F]FAA cleared rapidly from the blood within 20 min after injection with a plasma half-life of ~10 min. The spleen had the highest accumulation at 120 min (the only time point studied) with 11.65% injected dose (ID)/g, followed by the kidney (3.5% ID/g), liver (2.4% ID/g), intestine (1.9% ID/g), heart (1.55% ID/g), and lung (1.4% ID/g). The accumulation in the two tumors was 1.75% ID/g in the wild-type tumor and 1.55% ID/g in the HSV-tk-transduced tumor with tumor/blood ratios of 3.27 and 2.92, respectively. The similar tumor uptakes suggested that [^18^F]FAA is not a substrate for HSV-tk gene. Radioactivity in the blood and muscle was 0.53% ID/g and 0.75% ID/g, respectively. PET images were obtained at 30, 60, and 120 min after injection. The spleen exhibited the highest radioactivity. Both tumors were clearly visualized. No significant differences in images were observed at the three time points. No blocking experiment was performed. The authors suggested that further studies are necessary to understand the mechanism of tumor accumulation.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+2-fluoroadenosine+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2-fluoroadenosine+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2-fluoroadenosine+human)]

No publication is currently available.

## NIH Support

CA72896

## References

1 Dzeja P.P., Terzic A. (2003). Phosphotransfer networks and cellular energetics. J Exp Biol.
2 Kim C.G., Yang D.J., Kim E.E., Cherif A., Kuang L.R., Li C., Tansey W., Liu C.W., Li S.C., Wallace S., Podoloff D.A. (1996). Assessment of tumor cell proliferation using [18F]fluorodeoxyadenosine and[18F]fluoroethyluracil. J Pharm Sci.
3 Mikhailopulo I.A., Poopeiko N.E., Pricota T.I., Sivets G.G., Kvasyuk E.I., Balzarini J., De Clercq E. (1991). Synthesis and antiviral and cytostatic properties of 3'-deoxy-3'-fluoro- and 2'-azido-3'-fluoro-2',3'-dideoxy-D-ribofuranosides of natural heterocyclic bases. J Med Chem.
4 Pittillo R.F., Moncrief C., Brockman R.W., Chambers P. (1964). Antimicrobial Activity of 2-Fluoroadenosine and 2-Fluoroadenine. Antimicrobial Agents Chemother (Bethesda).
5 Secrist J.A., Shortnacy A.T., Montgomery J.A. (1988). Synthesis and biological evaluations of certain 2-halo-2'-substituted derivatives of 9-beta-D-arabinofuranosyladenine. J Med Chem.
6 Takahashi T., Kanazawa J., Akinaga S., Tamaoki T., Okabe M. (1999). Antitumor activity of 2-chloro-9-(2-deoxy-2-fluoro-beta-D-arabinofuranosyl) adenine, a novel deoxyadenosine analog, against human colon tumor xenografts by oral administration. Cancer Chemother Pharmacol.
7 Alauddin M.M., Shahinian A., Park R., Tohme M., Fissekis J.D., Conti P.S. (2007). Biodistribution and PET imaging of [(18)F]-fluoroadenosine derivatives. Nucl Med Biol.